# O-(2-[^18^F]Fluoroethyl)-L-tyrosine

Chemical name: | O-(2-[^18^F]Fluoroethyl)-L-tyrosine
Abbreviated name: | FET, [^18^F]FET
Synonym:
Agent category: | Compound
Target: | L-type amino acid transporter system and Na^+^-dependent system B^0^
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroethyl%20l%20tyrosine%20)]

A variety of [^11^C] and [^18^F] labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain (3). These amino acids are composed of naturally occurring amino acids such as, L-[^11^C]leucine, L-[^11^C]methionine (MET), and L-[^11^C]tyrosine and non-natural amino acids such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. There are also ^123^I-labeled amino acids used in imaging in oncology (1, 4, 5).

Some 20 amino acid transporter systems have been identified (1). Most of the amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and a sodium-dependent transporter system A but also a Na^+^-dependent system B^0^ (6). They are retained in tumor cells due to their higher metabolic activities including incorporation into proteins than most normal cells (1). Malignant transformation increases the use of amino acids for energy, protein synthesis and cell division. Tumor cells were found to have over-expressed transporter systems (7). L-[^11^C]MET, [^18^F]fluorotyrosine, L-[^11^C]leucine, and [^18^F]fluoro-α-methyl tyrosine have been widely used in detection of tumors (2, 6) but are not approved by the FDA. They are moved into cells by various amino acid transporters and are incorporated into proteins. The fraction of radiolabeled amino acid that is incorporated into protein is usually small compared to the total amount taken up into the cell. These natural amino acid images are based on amino acid transport and protein incorporation.

None of the non-natural amino acids is incorporated into proteins (2, 8). These amino acids are rapidly transported into tumor cells. They are retained inside the tumor cells because of their high cellular metabolism and their high activity of the amino acid transporters. Recently, a new L-tyrosine analog, O-(2-[^18^F]fluoroethyl)-L-tyrosine ([^18^F]FET), was synthesized and evaluated as an amino acid PET tracer for the detection of brain tumors with a higher specificity as compared with [^18^F]FDG. Therefore, [^18^F]FET could be a useful tracer in brain tumor imaging based solely on amino acid transport.

### Related Resource Links:

- Chapters in MICAD (Amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D))
- Gene information in NCBI (L-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=O-%20%282-%5BAll%20Fields%5D%20fluoroethyl%29%20l%20tyrosine%20and%20synthesis)]

[^18^F]FET was synthesized by a direct alkylation of tyrosine with [^18^F]fluoroethyltosylate as previously reported by Wester et al. (8). [^18^F]fluoroethyltosylate was prepared by [^18^F]fluorination of ethylene glycol-1,2-ditosylate with [^18^F] potassium Kryptofix complex. This two-step synthesis provided [^18^F]FET with a 40% overall radiochemical yield and a radiochemical purity >97% with a total synthesis time of 50 min.

An automated synthesis of [^18^F]FET was reported using O-(2-tosyloxyethyl)-N-trityl-L-tyrosine tert-butylester as a precursor for one-step nucleophilic [^18^F]fluorination in the presence of tetra-butyl ammonium hydrogen carbonate/carbonate (9). The specific activity of [^18^F]FET was 18 GBq/μmol (0.49 Ci/μmol) with a total synthesis time of 80 min and a radiochemical yield of 55-60%. This method provided a radiochemical purity >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=O-%20%282-%5BAll%20Fields%5D%20fluoroethyl%29%20l%20tyrosine%20and%20in%20vitro)]

[^18^F]FET was shown to be transported mainly (80%) by the L-type amino acid transporter system, which was inhibited by 2-amino-2-norbornanecarboxylic acid (BCH) and not incorporated into proteins in human SW707 colon carcinoma cells (10). [^18^F]FET showed a fast accumulation into SW707 cells for the first 6 min, followed by a plateau of nearly constant radioactivity up to 30 min. There was no significant accumulation of D-[^18^F]FET. [^18^F]FET was found to be transported into F98 rat gliomas similarly to L-[^3^H]methionine mainly by system L and also (30%) by the Na^+^-dependent system B^0^ (6). No significant incorporation of FET into proteins was detected.

[^18^F]FET showed a fast-increasing uptake into F98 rat glioma cells in the first 10 min (0.475%) in culture, followed by a plateau of nearly constant radioactivity up to 60 min of incubation (11). On the other hand, [^18^F]fluoro-2-deoxy-2-D-glucose (FDG) was increasingly accumulated into the cells over 60 min (1.07% at 60 min).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=O-%20%282-%5BAll%20Fields%5D%20fluoroethyl%29%20l%20tyrosine%20and%20rodentia)]

Biodistribution studies in mice bearing SW707 colon carcinomas showed a high uptake of radioactivity in the pancreas (18% injected dose (ID)/g) at 60 min after injection of [^18^F]FET (8). The brain (2.17% ID/g) and the tumors (6.37% ID/g) showed moderate uptakes of the tracer. Low radioactivity was observed in bone tissue, indicating little defluorination. The liver, kidney, and blood showed a fast distribution of [^18^F]FET, completed in less than 5 min. The other organs showed little elevated uptake with time. [^18^F]FET remained intact in the tissue homogenates of pancreas, brain, and tumor and plasma samples. No incorporation of [^18^F]FET into proteins was detected in the tissue homogenates.

The biodistribution of [^18^F]FET was determined in brain F98 glioma-bearing rats and compared with FDG (11). A moderate uptake and a long retention time of [^18^F]FET in most organs, such as kidneys, liver, lung, blood, and heart, whereas a low uptake were found in normal brain. The maximum uptake of [^18^F]FET and FDG in the F98 tumor was observed at 60 min after injection (1.49% and 2.77% ID/g), respectively. The tumor-to-brain ratios were 3.15 for [^18^F]FET and 1.44 for FDG. Both PET images and autoradiograms of [^18^F]FET showed high tracer uptake and contrast in the brain tumor, whereas FDG showed poor brain tumor images because of high uptake in the normal brain. [^18^F]FET seems to be a useful amino acid tracer for brain tumor imaging with PET.

[^18^F]FET did not accumulate significantly in inflammatory tissues (12). Tumor-infiltrated lymph nodes could be differentiated from inflammatory lymph nodes (13), and radiation necrosis could be differentiated from tumor recurrence (14). [^18^F]FET was found to be a better tracer than [^11^C]MET, [^18^F]fluorocholine, or FDG in these circumstances because [^18^F]FET does not accumulate in macrophages as compared with [^18^F]fluorocholine and FDG.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=O-%20%282-%5BAll%20Fields%5D%20fluoroethyl%29%20l%20tyrosine%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=O-%20%282-%5BAll%20Fields%5D%20fluoroethyl%29%20l%20tyrosine%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=O-%20%282-%5BAll%20Fields%5D%20fluoroethyl%29%20l%20tyrosine%20and%20human)]

Human dosimetry was estimated based on human dynamic PET scans after injection of 400 MBq (10.8 mCi) [^18^F]FET at 70 and 200 min (15). The urinary bladder received the highest dose (0.060 mGy/MBq or 222 mrad/mCi). Other organs, the uterus (0.022 mGy/MBq or 81 mrad/mCi) and kidney (0.020 mGy/MBq or 74 mrad/mCi), received moderate doses. No increased uptake was seen in the liver, bone, intestine, lung, heart, or pancreas. The effective dose was 0.0165 mSv/MBq (61 mrem/mCi). The effective dose based on biodistribution data of mice was estimated to be 0.009 mSv/MBq (33 mrem/mCi) (16).

A series of peripheral tumors were compared with [^18^F]FET and FDG PET scans in 38 cancer patients (17). [^18^F]FET was positive in 13 of 38 patients, whereas FDG was positive in 37 of 38 patients. However, in patients with squamous cell carcinomas, [^18^F]FET provided better discrimination than FDG between lesions and inflammatory tissues.

Initial clinical studies of [^18^F]FET in comparison with [^11^C]MET were carried out in 16 patients with intracerebral lesions, showing brain tumor images in 13 patients (18). There were few differences in uptake and image contrast between [^11^C]MET and [^18^F]FET. In a different study, 20 patients with suspected brain tumors were imaged by [^18^F]FET PET, 3-[^123^I]-iodo-α-methyl-L-tyrosine (IMT) SPECT, and magnetic resonance imaging (MRI) (19). [^18^F]FET and IMT showed similar uptakes in brain lesions. However, [^18^F]FET exhibited a significant higher tumor-to-brain ratio than IMT and an improved discrimination of anatomic structures over IMT. In a later study, [^18^F]FET PET improved the specificity of MRI from 53% to 94% in diagnostic assessment of cerebral gliomas in 31 patients (20). These and other studies [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=O-%20%282-%5BAll%20Fields%5D%20fluoroethyl%29%20l%20tyrosine%20and%20human)] have demonstrated that [^18^F]FET PET provides accurate delineation of brain tumor metastases, detection of brain tumor recurrence, and identification of brain lesions.

## References

1 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
2 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
5 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
6 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
7 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
8 Wester H.J., Herz M., Weber W., Heiss P., Senekowitsch-Schmidtke R., Schwaiger M., Stocklin G. (1999). Synthesis and radiopharmacology of O-(2-[18F]fluoroethyl)-L-tyrosine for tumor imaging. J Nucl Med.
9 Hamacher K., Coenen H.H. (2002). Efficient routine production of the 18F-labelled amino acid O-2-18F fluoroethyl-L-tyrosine. Appl Radiat Isot.
10 Heiss P., Mayer S., Herz M., Wester H.J., Schwaiger M., Senekowitsch-Schmidtke R. (1999). Investigation of transport mechanism and uptake kinetics of O-(2-[18F]fluoroethyl)-L-tyrosine in vitro and in vivo. J Nucl Med.
11 Wang H.E., Wu S.Y., Chang C.W., Liu R.S., Hwang L.C., Lee T.W., Chen J.C., Hwang J.J. (2005). Evaluation of F-18-labeled amino acid derivatives and [18F]FDG as PET probes in a brain tumor-bearing animal model. Nucl Med Biol.
12 Kaim A.H., Weber B., Kurrer M.O., Westera G., Schweitzer A., Gottschalk J., von Schulthess G.K., Buck A. (2002). (18)F-FDG and (18)F-FET uptake in experimental soft tissue infection. Eur J Nucl Med Mol Imaging.
13 Rau F.C., Weber W.A., Wester H.J., Herz M., Becker I., Kruger A., Schwaiger M., Senekowitsch-Schmidtke R. (2002). O-(2-[(18)F]Fluoroethyl)- L-tyrosine (FET): a tracer for differentiation of tumour from inflammation in murine lymph nodes. Eur J Nucl Med Mol Imaging.
14 Spaeth N., Wyss M.T., Weber B., Scheidegger S., Lutz A., Verwey J., Radovanovic I., Pahnke J., Wild D., Westera G., Weishaupt D., Hermann D.M., Kaser-Hotz B., Aguzzi A., Buck A. (2004). Uptake of 18F-fluorocholine, 18F-fluoroethyl-L-tyrosine, and 18F-FDG in acute cerebral radiation injury in the rat: implications for separation of radiation necrosis from tumor recurrence. J Nucl Med.
15 Pauleit D., Floeth F., Herzog H., Hamacher K., Tellmann L., Muller H.W., Coenen H.H., Langen K.J. (2003). Whole-body distribution and dosimetry of O-(2-[18F]fluoroethyl)-L-tyrosine. Eur J Nucl Med Mol Imaging.
16 Tang G., Tang X., Wang M., Luo L., Gan M. (2004). Radiation dosimetry of O-(3-[18F]fluoropropyl)-L-tyrosine as oncologic PET tracer based on the mice distribution data. Appl Radiat Isot.
17 Pauleit D., Stoffels G., Schaden W., Hamacher K., Bauer D., Tellmann L., Herzog H., Broer S., Coenen H.H., Langen K.J. (2005). PET with O-(2-18F-Fluoroethyl)-L-Tyrosine in peripheral tumors: first clinical results. J Nucl Med.
18 Weber W.A., Wester H.J., Grosu A.L., Herz M., Dzewas B., Feldmann H.J., Molls M., Stocklin G., Schwaiger M. (2000). O-(2-[18F]fluoroethyl)-L-tyrosine and L-[methyl-11C]methionine uptake in brain tumours: initial results of a comparative study. Eur J Nucl Med.
19 Pauleit D., Floeth F., Tellmann L., Hamacher K., Hautzel H., Muller H.W., Coenen H.H., Langen K.J. (2004). Comparison of O-(2-18F-fluoroethyl)-L-tyrosine PET and 3-123I-iodo-alpha-methyl-L-tyrosine SPECT in brain tumors. J Nucl Med.
20 Pauleit D., Floeth F., Hamacher K., Riemenschneider M.J., Reifenberger G., Muller H.W., Zilles K., Coenen H.H., Langen K.J. (2005). O-(2-[18F]fluoroethyl)-L-tyrosine PET combined with MRI improves the diagnostic assessment of cerebral gliomas. Brain.